# Gadolinium-Diethylenetriamine pentaacetic acid-Leu-Ile-Lys-Lys-Pro-Phe

Chemical name: | Gadolinium-Diethylenetriamine pentaacetic acid-Leu-Ile-Lys-Lys-Pro-Phe
Abbreviated name: | Gd-DTPA-g-R826
Synonym:
Agent category: | Peptide
Target: | Phosphatidylserine
Target category: | Acceptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal: | Gadolinium, Gd
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=R826)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally (1). Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules, which comprise >80% of most soft tissues. The contrast of proton MRI images depends mainly on the density of nuclear proton spins, the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the use of contrast agents. Most contrast agents affect the T1 and T2 relaxation of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (2). Cross-linked iron oxide (CLIO) and other iron oxide formulations affect T2 primarily and lead to a decreased signal. On the other hand, the paramagnetic T1 agents, such as gadolinium (Gd^3+^), and manganese (Mn^2+^), accelerate T1 relaxation and lead to brighter contrast images.

Apoptosis (programmed cell death) plays an important role in the pathophysiology of many diseases, such as cancer, neurodegenerative disorders, vascular disorders, and chronic hepatitis, as well as in the biology of normal cells like epithelial cells and immune cells (3). During apoptosis, there is rapid redistribution of phosphatidylserine from the inner membrane leaflet to the outer membrane leaflet, exposing the anionic head group of PS. PS is also accessible for annexin V binding in apoptosis and necrosis because of disruption of the plasma membrane. Annexin V binds to PS with high affinity (dissociation constant = 7 nM). Annexin V has been radiolabeled with ^123^I, ^124^I, and ^99m^Tc for single-photon emission computed tomography imaging (4-6). Recently, annexin V was successfully labeled with ^18^F (7, 8), and ^18^F-labeled annexin V is being developed as a positron emission tomography agent for imaging apoptosis as well as necrosis. Cy5.5-annexin V and quantum dot (QD)-annexin V (9) have been evaluated as optical probes for near-infrared (NIR) imaging. Various bimodal annexin V–conjugated nanoparticles have been developed for imaging apoptosis, such as annexin V-CLIO-Cy5.5 and annexin V-QD-gadolinium for NIR and MRI imaging (10, 11).

A cyclic peptide, Cys-Leu-Ile-Lys-Lys-Pro-Phe-Cys, was identified with phage screening against PS (12). Leu-Ile-Lys-Lys-Pro-Phe (R826) was synthesized and conjugated to the 8-amino-3,6-dioxaoctanoyl linker to form g-R826, which was conjugated with 2-(4-isothiocyanatobenzyl)-diethylenetriamine pentaacetic acid (p-SCN-Bn-DTPA) to form DTPA-g-R826 for labeling with Gd for MRI of PS in apoptosis.

### Related Resource Links:

- Chapters in MICAD (Annexin V (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Annexin%20V+AND+micad%5Bbook%5D))
- Gene information in NCBI (Annexin V (http://www.ncbi.nlm.nih.gov/gene/308))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Annexin V (http://www.ncbi.nlm.nih.gov/omim/131230))
- Clinical trials (Annexin V (http://www.clinicaltrials.gov/ct2/results?term=Annexin+V+))
- Drug information in FDA (Annexin V (http://google2.fda.gov/search?q=annexin+V&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=3&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=R826%20and%20synthesis)]

R826 peptide (with two Lys, protected with trifluoroacetic acid, and attached to 8-amino-3,6-dioxaoctanoyl at the N-terminus) was conjugated with two molar equivalents of p-SCN-Bn-DTPA for 48 h at room temperature (12). After removal of the protecting groups, DTPA-g-R826 was purified with dialysis and column chromatography. GdCl_3_ was added to a solution of DTPA-g-R826 and incubated for 24 h at room temperature. Gd-DTPA-g-R826 was purified with dialysis. The scrambled sequence of R826 (R826.Sc) was also conjugated to form Gd-DTPA-g-R826.Sc as a nonspecific control. The mass of Gd-DTPA-g-R826 was confirmed with mass spectroscopy. Longitudinal (r_1_) relaxivity values (nuclear magnetic resonance efficiency expressed in mM^-1^s^-1^) of Gd-DTPA-g-R826, Gd-DTPA-g-R826.Sc, and Gd-DTPA were 10.5, 10.5, and 3.8 measured at 0.3 T, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=R826%20and%20in%20vitro)]

Burtea et al. (12) performed in vitro binding of Gd-DTPA-g-R826 (0.4 mM) to apoptotic Jurkat T cells. Gd concentrations were 400 and 140 nmol Gd per gram of cells for the apoptotic cells and control cells, respectively. Less than 5 nM Gd/g was observed in the apoptotic cells and control cells for Gd-DTPA-g-R826.Sc and Gd-DTPA. Caspase-3 activity was approximately nine times higher in the apoptotic cells than in the control cells. R826 exhibited a 50% inhibition concentration value of 14.8 nM using biotinylated annexin V with the apoptotic cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=R826%20and%20rodentia)]

Burtea et al. (12) performed in vivo MRI in apolipoprotein E–deficient (apoE^-/-^) mice after injection with 0.06 mmol/kg Gd-DTPA-g-R826 (n = 11), Gd-DTPA-g-R826.Sc (n = 4), or Gd-DTPA (n = 5). There was 132% enhancement in MRI signal intensity (ΔSNR) in the aortic wall at 10 min after injection. The ΔSNR remained constant (111%) for up to 61 min of imaging. Gd-DTPA-g-R826.Sc exhibited ΔSNR of 93% and 68% at 25 and 60 min, respectively. Gd-DTPA produced ΔSNR of 89% and 45% at 10 and 60 min, respectively. Immunohistological staining of the aorta sections of apoE^-/-^ mice confirmed the presence of atherosclerotic lesions with extensive expression of PS. In mice with liver apoptosis induced with anti-Fas antibody, Gd-DTPA-g-R826 (n = 11) showed ΔSNR of 94% at 60 min and 60% at 90 min after injection, whereas healthy liver (n = 7) showed ΔSNR of 38% during the first 8 min, which decreased to <5% at 60 min after injection. Pretreatment with 0.1 mmol/kg R826 (10 min before Gd-DTPA-g-R826 injection) reduced the ΔSNR to <30% from 10–60 min after injection (n = 6). Gd-DTPA-g-R826.Sc (n = 8) showed ΔSNR of <40% at 10–60 min after injection in apoptotic and normal livers. Gd-DTPA (n = 7) showed ΔSNR of 20–30% R832 at 10 min and decreased to <5% at 60 min after injection. Immunohistological staining of the apoptotic liver sections confirmed the presence of extensive expression of PS.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=R826%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=R826%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=R826%20and%20human)]

No publication is currently available.

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Burtea, C., S. Laurent, L. Vander Elst, and R.N. Muller, Contrast agents: magnetic resonance. Handb Exp Pharmacol, 2008(185 Pt 1): p. 135-65.
3 Thompson C.B. (1995). Apoptosis in the pathogenesis and treatment of disease. Science.
4 Blankenberg F.G. (2004). Recent advances in the imaging of programmed cell death. Curr Pharm Des.
5 Lahorte C., Slegers G., Philippe J., Van de Wiele C., Dierckx R.A. (2001). Synthesis and in vitro evaluation of 123I-labelled human recombinant annexin V. Biomol Eng.
6 Keen H.G., Dekker B.A., Disley L., Hastings D., Lyons S., Reader A.J., Ottewell P., Watson A., Zweit J. (2005). Imaging apoptosis in vivo using 124I-annexin V and PET. Nucl Med Biol.
7 Toretsky J., Levenson A., Weinberg I.N., Tait J.F., Uren A., Mease R.C. (2004). Preparation of F-18 labeled annexin V: a potential PET radiopharmaceutical for imaging cell death. Nucl Med Biol.
8 Zijlstra S., Gunawan J., Burchert W. (2003). Synthesis and evaluation of a 18F-labelled recombinant annexin-V derivative, for identification and quantification of apoptotic cells with PET. Appl Radiat Isot.
9 Schellenberger E.A., Sosnovik D., Weissleder R., Josephson L. (2004). Magneto/optical annexin V, a multimodal protein. Bioconjug Chem.
10 Prinzen L., Miserus R.J., Dirksen A., Hackeng T.M., Deckers N., Bitsch N.J., Megens R.T., Douma K., Heemskerk J.W., Kooi M.E., Frederik P.M., Slaaf D.W., van Zandvoort M.A., Reutelingsperger C.P. (2007). Optical and magnetic resonance imaging of cell death and platelet activation using annexin a5-functionalized quantum dots. Nano Lett.
11 van Tilborg G.A., Mulder W.J., Chin P.T., Storm G., Reutelingsperger C.P., Nicolay K., Strijkers G.J. (2006). Annexin A5-conjugated quantum dots with a paramagnetic lipidic coating for the multimodal detection of apoptotic cells. Bioconjug Chem.
12 Burtea C., Laurent S., Lancelot E., Ballet S., Murariu O., Rousseaux O., Port M., Vander Elst L., Corot C., Muller R.N. (2009). Peptidic targeting of phosphatidylserine for the MRI detection of apoptosis in atherosclerotic plaques. Mol Pharm.